# 3-(6-Methyl-pyridin-2-ylethynyl)-cyclohex-2-enone-O-^11^C-methyl-oxime

Chemical name: | 3-(6-Methyl-pyridin-2-ylethynyl)-cyclohex-2-enone-O-^11^C-methyl-oxime
Abbreviated name: | [^11^C]ABP688
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate receptor subtype 5 (mGlu5)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-ABP688%5BAll%20Fields%5D)]

3-(6-Methyl-pyridin-2-ylethynyl)-cyclohex-2-enone-O-^11^C-methyl-oxime ([^11^C]ABP688) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate receptor subtype 5 (mGlu5) in the central nervous system (CNS) (1).

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (2). Glutamate produces its excitatory effects by acting on cell surface ionotropic glutamate or metabotropic glutamate (mGlu) receptors (3). The mGlu receptors are G-protein-coupled receptors, and there are eight mGlu receptor subtypes that are further subdivided into groups I, II, and III. The group I receptors include mGlu1 and mGlu5, and they are mostly in postsynaptic locations. The mGlu5 receptors are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors are coupled to phospholipase C and up- or down-regulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states. They thus are attractive targets for therapeutic drug development.

PET and single-photon emission tomography of radioligands targeting mGlu5 receptors can visualize and study the CNS mGlu5 receptors in normal and pathologic states. Some mGlu5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or a high metabolism (1, 4). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP) and its methyl analog M-MPEP have been identified as potent and highly selective noncompetitive antagonists for mGlu5. With MPEP used as a template, [^11^C]ABP688 was synthesized and developed as a potential PET agent without shortcomings similar to those for other agents (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-ABP688%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Kessler (5) designed a four-step reaction sequence for the synthesis of desmethyl-ABP688 as a precursor of [^11^C]ABP688 radiosynthesis. ABP688 was labeled with ^11^C by reaction of the sodium salt of desmethyl-ABP688 in anhydrous dimethylformamide with [^11^C]methyl iodide at 90 °C for 5 min (1). The product was purified by semipreparative high-performance liquid chromatography (HPLC). The prepared [^11^C]ABP688 was >95% radiochemically pure, the radiochemical yield was 35 ± 8%, and the specific activity was 100-200 GBq (2.7-8.1 Ci)/μmol. The total synthesis time was reported to be 45-50 min. ^13^C-Nuclear magnetic resonance (NMR) gave a peak signal for the O-methyl C atom at 61.5 ppm. Mass spectrometry indicated that the molecular ion peak ([M + 1]^+^) was at m/z 242. NMR data showed an E/Z isomeric ratio of at least 6:1. The E-isomer was the most potent isomer and could be consistently obtained as the major component (>10:1) when the desmethyl-ABP688 sodium salt was preheated to 90 °C and [^11^C]methyl iodide was then added at that temperature.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-ABP688%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

The distribution coefficient (Log D) of [^11^C]ABP688, as determined by Ametamey et al. (1), was 2.4 ± 0.1 (n = 3). [^11^C]ABP688 was stable in human plasma in vitro at 37 °C for at least 60 min. In vitro binding of [^11^C]ABP688 was studied in rat brain tissue membranes. Saturation studies indicated that the receptor binding was saturable, and the Scatchard plot indicated a single high-affinity binding site with a K_D_ of 1.7 ± 0.2 nM (n = 3). The B_max_ was 231 ± 18 fmol/mg of protein. Ex vivo autoradiography of rat brain showed that the brain uptake of [^11^C]ABP688 was highly selective, with high radioactivity concentrations in known mGlu5-rich regions and negligible radioactivity in mGlu5-poor regions. Autoradiography in wild-type (wt) mice showed a similar specific brain uptake of [^11^C]ABP688. Studies in mGlu5-knockout (ko) mice showed homogeneous and markedly reduced accumulation of radioactivity throughout the brain.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-ABP688%5BAll%20Fields%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Ametamey et al. (1) performed biodistribution studies of [^11^C]ABP688 in rats. The rats received doses of 50-450 MBq (1.4-12.2 mCi) in 0.4-3.5 nM and were decapitated 30 min after injection. The kidney and liver had the highest radioactivity localization, with 0.2 and 0.18% of injected dose normalized to body weight (% ID norm/g), respectively. The lung, blood, muscle, and bone had <0.1% ID norm/g. In the brain, relatively high amounts of radioactivity were found in mGlu5-rich regions such as the hippocampus, striatum, and cortex, whereas relatively low amounts of radioactivity were found in mGlu5-poor regions (cerebellum). The striatum/cerebellum, hippocampus/cerebellum, and cortex/cerebellum ratios (n = 3) were 6.6 ± 0.1, 5.4 ± 0.1, and 4.6 ± 0.1, respectively. In a blocking experiment in which 1.0 mg/kg M-MPEP (mGlu5 antagonist) was injected together with [^11^C]ABP688, up to 80% of radioactivity uptake was blocked in the hippocampus and striatum. No blocking effects were found in the cerebellum. Under blocking conditions, the liver showed an increase in radioactivity uptake. No blocking effects were observed in all other peripheral organs. HPLC analysis of whole-brain extracts showed that >95% of [^11^C]ABP688 remained unchanged 30 min after injection. About 75% of the radioactivity in the blood and 95% of the radioactivity in the urine was radiolabeled polar metabolites that could not cross the blood-brain barrier. Brain PET imaging (90 min) was performed on rats that had received doses of 18-22 MBq (0.49-0.59 mCi) in 1-3 nmol. Images showed specific radioactivity localization in mGlu5-rich regions such as the caudate putamen and hippocampus. This localization was inhibited by coadministration of M-MPEP.

Similar biodistribution studies in wt and ko mice were performed by Ametamey et al. (1). The mice received doses of 50-350 MBq (1.4-9.5 mCi) in 0.5-2.5 nM and were decapitated 20 min after administration. Brain radioactivity distribution patterns in mGlu5-rich regions in wt mice were similar to those in the rat brain, whereas localization of radioactivity in all of the brain regions was significantly less in the ko mice. Brain PET imaging was performed in mice that received doses of 18-22 MBq (0.49-0.59 mCi) in 1-3 nmol. Brain images from wt mice showed localization of radioactivity similar to that in the rats, with the highest amounts of radioactivity in the striatum and hippocampus. Radioactivity ratios for the hippocampus/cerebellum and striatum/cerebellum were >2. The ko mice showed homogeneous distribution of radioactivity throughout the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-ABP688%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

Put non-human primates here.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-ABP688%29%20AND%20human)]

No publication is currently available.

## References

1 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
2 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
3 Slassi A., Isaac M., Edwards L., Minidis A., Wensbo D., Mattsson J., Nilsson K., Raboisson P., McLeod D., Stormann T.M., Hammerland L.G., Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
4 Hamill T.G., Krause S., Ryan C., Bonnefous C., Govek S., Seiders T.J., Cosford N.D., Roppe J., Kamenecka T., Patel S., Gibson R.E., Sanabria S., Riffel K., Eng W., King C., Yang X., Green M.D., O'Malley S.S., Hargreaves R., Burns H.D. (2005). Synthesis, characterization, and first successful monkey imaging studies of metabotropic glutamate receptor subtype 5 (mGluR5) PET radiotracers. Synapse.
5 Kessler L.J. (2006). Development of novel ligands for PET imaging of metabotropic glutamate receptor subtype 5 (mGluR5), Swiss Federal Institute of Technology Zurich: Zurich.